# ^125^I-Anti-malondialdehyde-modified low-density lipoprotein monoclonal antibody

Chemical name: | ^125^I-Anti-malondialdehyde-modified low-density lipoprotein monoclonal antibody
Abbreviated name: | ^125^I-MDA2
Synonym:
Agent category: | Antibody
Target: | Malondialdehyde-modified low-density lipoprotein (MDA-LDL)
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=44888831), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=217035086) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=338) for more information about apolipoprotein B.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2)]

Apolipoprotein E (apoE) is essential for the normal catabolism of triglyceride-rich lipoprotein chylomicrons (lipoprotein particles) (1). Oxidation of low-density lipoprotein (LDL) generates a number of highly reactive short chain-length aldehydic fragments of oxidized fatty acids capable of conjugating with lysine residues of apoliprotein B and other proteins. Oxidized LDL is present in atherosclerotic lesions and is essential for formation of foam cells in atherosclerotic plaques. During atherogenic conditions, depositions of lipids and extracellular matrix proteins on the endothelial cell surfaces of the aorta and cells lead to the development of atherosclerotic plaques (2), which may erode and rupture. MDA2 is a murine monoclonal antibody (mAb) to malondialdehyde-lysine epitopes of MDA-LDL and other oxidatively modified proteins but not to normal LDL (3). Tsimikas and colleagues (4-6) have studied ^125^I-MDA2 for imaging atherosclerotic plaques in small animals.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+synthesis)]

MDA2 was labeled with ^125^I via the lactoperoxidase/glucose oxidase method (5). ^125^I-MDA2 had a specific activity of 555 MBq/µmol (15 mCi/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+in+vitro)]

^125^I-MDA2 has been shown to bind specifically to human MDA-LDL but not to normal human LDL, high-density lipoprotein, very low-density lipoprotein, or bovine serum albumin (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+rodentia)]

Tsimikas et al. (6) measured accumulation of ^125^I-MDA2 in the aorta of 6-month-old LDLR^-/-^ knockout mice that were fed a high-fat, high-cholesterol diet (n = 9 mice), a normal chow diet (n = 8 mice), or a normal chow diet supplemented with vitamin E+C (n = 9 mice) for 6 months. The aortic weight was 35, 18, and 15 mg, respectively. The percent of injected dose was 0.14 ± 0.03, 0.03 ± 0.01, and 0.03 ± 0.01, respectivelyat 24 h after injection. There was a high amount of oxidized LDL in the aorta of mice fed the high-fat diet.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(dog+or+pig+or+sheep+or+rabbit))]

Tsimikas et al. (5) performed ex vivo assessment of ^125^I-MDA2 for atherosclerotic lesions in LDL receptor–deficient Watanabe heritable hyperlipidemic rabbits (WHHL, n = 7) and normal New Zealand white rabbits (NZW, n = 2) at 24 h after injection. ^125^I-Halb, an isotype-matched irrelevant mAb that binds to human albumin, was used as a control. The blood half-life was 12 h for ^125^I-MDA2 and 9 h for ^125^I-Halb in both WHHL and NZW rabbits. Aortic autoradiography was performed, and the mean uptake of mAbs was measured as the percent of injected dose per gram (% ID/g) of aortic tissueat 24 h after injection. Mean uptake of ^125^I-MDA2 in the entire aorta (0.09% ID/g) was 17.4-fold higher in WHHL than in NZW aortas (P < 0.001) and 2.8-fold higher than mean uptake of ^125^I-Halb in the WHHL aortas (P < 0.01). ^125^I-MDA2 also had higher specificity for lesioned areas than did ^125^I-Halb (plaque/normal ratio, 6.3 versus 2.9, P < 0.001). Autoradiographic analysis of aortasat 24 h after injection from NZW rabbits injected with ^125^I-MDA2 did not yield any visible signal. Injection of 10 mg MDA-LDL 24 h after injection of ^125^I-MDA2 in WHHL rabbits reduced the residual blood radioactivity from 31% to 7.5% (P < 0.001). There was no significant difference in the aortic accumulation in the two groups; however, there was an improvement in the plaque/blood ratio from 0.6 to 1.4. Autoradiographs of aortas of ^125^I-MDA2-injected WHHL rabbits revealed uptake in lipid-stained lesions with an absence of signal in adjacent normal arterial tissue. Immunostaining of WHHL lesions revealed that uptake was highest in areas with abundant foam cells and in lipid-rich necrotic core areas.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+human)]

No publication is currently available.

## NIH Support

HL07444, HL03793, HL14197, HL05989

## References

1 Eichner J.E., Dunn S.T., Perveen G., Thompson D.M., Stewart K.E., Stroehla B.C. (2002). Apolipoprotein E polymorphism and cardiovascular disease: a HuGE review. Am J Epidemiol.
2 Libby P., Ridker P.M., Maseri A. (2002). Inflammation and atherosclerosis. Circulation.
3 Palinski W., Yla-Herttuala S., Rosenfeld M.E., Butler S.W., Socher S.A., Parthasarathy S., Curtiss L.K., Witztum J.L. (1990). Antisera and monoclonal antibodies specific for epitopes generated during oxidative modification of low density lipoprotein. Arteriosclerosis.
4 Tsimikas S. (2002). Noninvasive imaging of oxidized low-density lipoprotein in atherosclerotic plaques with tagged oxidation-specific antibodies. Am J Cardiol.
5 Tsimikas S., Palinski W., Halpern S.E., Yeung D.W., Curtiss L.K., Witztum J.L. (1999). Radiolabeled MDA2, an oxidation-specific, monoclonal antibody, identifies native atherosclerotic lesions in vivo. J Nucl Cardiol.
6 Tsimikas S., Shortal B.P., Witztum J.L., Palinski W. (2000). In vivo uptake of radiolabeled MDA2, an oxidation-specific monoclonal antibody, provides an accurate measure of atherosclerotic lesions rich in oxidized LDL and is highly sensitive to their regression. Arterioscler Thromb Vasc Biol.